# ^177^Lu-Labeled humanized monoclonal antibody against human epidermal growth factor receptor 2

Chemical name: | ^177^Lu-Labeled humanized monoclonal antibody against human epidermal growth factor receptor 2
Abbreviated name: | [^177^Lu]Pertuzumab
Synonym: | ^177^Lu-labeled Omnitrag^®^; ^177^Lu-labeled rhuMAb 2C4
Agent Category: | Humanized monoclonal antibody
Target: | Human epidermal growth factor receptor 2 (HER2 or HrbB2/neu)
Target Category: | Binding
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of Signal/Contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the human nucleotide and protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=194688152) sequence of HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177+Lu+pertuzumab)]

The human epidermal growth factor (EGF) receptor 2 (HER2 or Erb2/neu) is known to be overexpressed in cells of certain cancers and to play a key role in promoting the growth and proliferation of primary and metastasized cancer cells, particularly in breast, ovarian, and urinary bladder cancers (1-4). HER2 is a glycoprotein that belongs to the EGF receptor (EGFR or ErbB1) family (for details regarding other HER or ErbB receptors and their ligands, see Friedlander et al. and Adams et al. (5, 6)). The ErbB receptors have four domains (designated I to IV): an extracellular region, a membrane-spanning region, an intracellular tyrosine kinase (TK), and a noncatalytic domain (7). Under normal conditions the EGFR and ErbB exist as monomers, but the binding of a ligand to the extracellular domain of the receptor results in conformational changes that promote the interaction of receptor domains I and III (7, 8). This interaction between two receptor domains leads to the formation of homodimers or heterodimers of the receptor and activation of the intracellular tyrosine kinase (TK). Subsequently, a complex intracellular signaling pathway may be activated, which results in malignant transformation of cells, cancer progression and survival, possible resistance to anticancer drugs, and the formation of tumors (6). In addition, overexpression or mutations of the ErbB1 or ErbB2 receptors have also been shown to promote oncogenic transformations of cells (5).

Among the ErbB receptors, ErbB2 has been shown to be the preferred receptor for the formation of heterodimers with other ErbBs (ErbB1, ErbB3, and ErbB4) because it has an open extracellular domain confirmation that facilitates the formation of potent, mitogenic heterodimers (5). Formation of the ErbB2/ErbB3 heterodimers has been reported in breast, prostate, lung, and colorectal cancers (5, 9-12). Because ErbB receptors have been shown to have a prominent role in the development of cancers, these receptors have been targeted with different antibodies (Abs) for the molecular therapy of this disease (5). Among the various Abs directed against the EGF/ErbB receptor, trastuzumab and pertuzumab specifically bind to and inhibit ErbB2 receptor activity (5).

Trastuzumab is a humanized monoclonal antibody (MAb) that inhibits cell proliferation by binding to the extracellular domain of the ErbB2 receptor and by blocking activation of the intracellular TK; however, the exact mode by which it inhibits the TK is unknown, and several mechanisms have been proposed for its activity (5, 13). This MAb is commercially available in the United States and has been approved (http://www.fda.gov/cder/foi/label/2008/103792s5175lbl.pdf) by the United States Food and Drug Administration for the treatment of breast cancer; some patients undergoing treatment with this MAb develop resistance against it or may experience cardiac toxicity (5). Pertuzumab is a new class of humanized MAbs against ErbB2 and is known as a receptor dimerization inhibitor. On binding to the dimerization domain of the ErbB2 receptor, pertuzumab sterically hinders receptor dimerization and inhibits the signal transduction pathway (7). It has been tested in vitro and in preclinical animal studies, and it is being evaluated in several clinical trials (http://clinicaltrials.gov/ct2/results?term=pertuzumab) to treat a variety of cancers as a monotherapy or in combination with other drugs and MAbs (14-19). Pertuzumab has been labeled with radioactive lutetium (^177^Lu) to obtain [^177^Lu]pertuzumab and used for biodistribution and imaging studies in mice (20, 21).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177+Lu+pertuzumab+synthesis)]

The synthesis, development, purification, and characterization of pertuzumab have been described in detail by Adams et al. (6).

Pertuzumab was radiolabeled as described by Persson et al. (20). Briefly, the MAb was conjugated to 2-(p-isothiocyanatobenzyl)-cyclohexyl-diethylenetriamine pentaacetic acid (CHX-A DTPA) in 0.7 M borate buffer (pH 9.2) overnight at 37°C. The conjugated MAb was purified on a NAP-5 size exclusion column in sodium acetate buffer (pH 5.5) and divided into ten batches for storage (the storage conditions were not described) until required for chelation with ^177^Lu. Chelation was performed for 30 min at room temperature, and purity of the chelated product was checked with instant thin-layer chromatography (ITLC). Chelation efficiency of the reaction was reported to be ~90%, and the product purity was ~99%. The Rf values for the various products of the chelation reaction on ITLC analysis were not provided in the publication. The specific activity of [^177^Lu]pertuzumab used for the in vitro studies was reported to be 1 MBq/pmol Ab (0.027 mCi/pmol Ab). For imaging studies the specific activity of [^177^Lu]pertuzumab was 45 MBq/pmol Ab (1.21 mCi/pmol Ab). The stability of ^177^Lu chelated to pertuzumab was reported to be 96 ± 5% when stored overnight in presence of excess ethylenediaminetetraactetate. When stored in phosphate-buffered saline the stability of chelated ^177^Lu was 93 ± 4% at 37°C and 100% at 4°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177+Lu+pertuzumab+in+vitro)]

The dissociation constant (K_d_) for native pertuzumab and CHX-conjugated pertuzumab was determined with Biacore analysis using a CM5 Sensor Chip with the immobilized HER2 receptor (20). The native pertuzumab had a K_d_ of 2.2±0.4 nM, and the CHX-conjugated MAb had a K_d_ of 1.8 ± 1.1 nM. The affinity constant was determined to be 4.1 ± 0.7 nM using a saturation experiment with SKOV-3 cells exposed to [^177^Lu]pertuzumab. The [^177^Lu]pertuzumab retention in the SKOV-3 cells was 90 ± 2% after 20 h and dropped to 51 ± 3% at 90 h. Native pertuzumab was reported to block the uptake of [^177^Lu]pertuzumab by the SKOV-3 cells, indicating that the labeled MAb was specific for HER2 (20).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177+Lu+pertuzumab+rodentia)]

The biodistribution (n = 12 animals) and imaging (n = 2 animals) characteristics of [^177^Lu]pertuzumab were studied in Balb/c (nu/nu) mice bearing SKOV-3 cell tumors on the right hind leg (20). For the biodistribution study the mice were euthanized 1, 3, and 7 days after administration of [^177^Lu]pertuzumab, and various organs (blood, heart, skin, bone, lungs, thyroid, liver, spleen, kidneys, and bladder) were harvested to determine uptake of the label. Maximum tumor uptake of the label was reported at 3 days with a tumor/blood ratio of ~6.7; this ratio increased to ~10 at day 7 primarily because the label in the blood was reduced to ~1.5% of the injected dose/gram tissue (% ID/g) from ~3% ID/g at day 3. Among all organs, the thyroid showed maximum retention of radioactivity after day 1 (8.7 ± 2.4% ID/g compared to 1–3% ID/g for other organs), which gradually decreased to ~1% ID/g, similar to the other organs, by day 7. Imaging was performed 1 day after administration of [^177^Lu]pertuzumab, and the radioactivity was primarily accumulated in the hind leg tumors (tumor/background ratios were 29 and 24 for the two animals, respectively).

In another study, mice (n = 9) bearing SKOV-3 tumors in the right front leg were treated with [^177^Lu]pertuzumab (20). To investigate specificity of the labeled MAb, of the four of nine mice were injected with an excess of unlabeled pertuzumab 30 min before the [^177^Lu]pertuzumab treatment. All the mice were euthanized, and the organs were harvested as detailed above to determine radioactivity accumulation in the tumors and organs. Little difference was reported in the radioactivity distribution in the various organs of the blocked and non-blocked mice. However, the tumors in the non-blocked mice showed ~4.4-fold greater accumulation of radioactivity compared with tumors from the blocked mice.

In another study, mice (n = 4/ time point) bearing SKOV-3 cell tumors were injected with [^177^Lu]pertuzumab and then euthanized at 8 h and 1, 3, 5, 7, and 14 d after injection (21). The tumors and various organs from the animals were harvested, and the accumulated radioactivity was determined. At 8 h after injection of [^177^Lu]pertuzumab, the tumor/blood ratio was 1.4, and this ratio increased to 19 after 14 days because the radioactivity decreased in the blood during this period.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pertuzumab+non+primate+animals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pertuzumab+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pertuzumab+humans)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Tewari K.S., Kyshtoobayeva A.S., Mehta R.S., Yu I.R., Burger R.A., DiSaia P.J., Fruehauf J.P. (2000). Biomarker conservation in primary and metastatic epithelial ovarian cancer. Gynecol Oncol.
2 Menard S., Casalini P., Campiglio M., Pupa S.M., Tagliabue E. (2004). Role of HER2/neu in tumor progression and therapy. Cell Mol Life Sci.
3 Gardmark T., Wester K., De la Torre M., Carlsson J., Malmstrom P.U. (2005). Analysis of HER2 expression in primary urinary bladder carcinoma and corresponding metastases. BJU Int.
4 Carlsson J., Nordgren H., Sjostrom J., Wester K., Villman K., Bengtsson N.O., Ostenstad B., Lundqvist H., Blomqvist C. (2004). HER2 expression in breast cancer primary tumours and corresponding metastases. Original data and literature review. Br J Cancer.
5 Friedlander E., Barok M., Szollosi J., Vereb G. (2008). ErbB-directed immunotherapy: antibodies in current practice and promising new agents. Immunol Lett.
6 Adams C.W., Allison D.E., Flagella K., Presta L., Clarke J., Dybdal N., McKeever K., Sliwkowski M.X. (2006). Humanization of a recombinant monoclonal antibody to produce a therapeutic HER dimerization inhibitor, pertuzumab. Cancer Immunol Immunother.
7 Franklin M.C., Carey K.D., Vajdos F.F., Leahy D.J., de Vos A.M., Sliwkowski M.X. (2004). Insights into ErbB signaling from the structure of the ErbB2-pertuzumab complex. Cancer Cell.
8 Ferguson K.M. (2004). Active and inactive conformations of the epidermal growth factor receptor. Biochem Soc Trans.
9 Gollamudi M., Nethery D., Liu J., Kern J.A. (2004). Autocrine activation of ErbB2/ErbB3 receptor complex by NRG-1 in non-small cell lung cancer cell lines. Lung Cancer.
10 Perez-Nadales E., Lloyd A.C. (2004). Essential function for ErbB3 in breast cancer proliferation. Breast Cancer Res.
11 Vakar-Lopez F., Cheng C.J., Kim J., Shi G.G., Troncoso P., Tu S.M., Yu-Lee L.Y., Lin S.H. (2004). Up-regulation of MDA-BF-1, a secreted isoform of ErbB3, in metastatic prostate cancer cells and activated osteoblasts in bone marrow. J Pathol.
12 Maurer C.A., Friess H., Kretschmann B., Zimmermann A., Stauffer A., Baer H.U., Korc M., Buchler M.W. (1998). Increased expression of erbB3 in colorectal cancer is associated with concomitant increase in the level of erbB2. Hum Pathol.
13 Bria E., Cuppone F., Milella M., Verma S., Carlini P., Nistico C., Vaccaro V., Rossi A., Tonini G., Cognetti F., Terzoli E. (2008). Trastuzumab cardiotoxicity: biological hypotheses and clinical open issues. Expert Opin Biol Ther.
14 Agus D.B., Sweeney C.J., Morris M.J., Mendelson D.S., McNeel D.G., Ahmann F.R., Wang J., Derynck M.K., Ng K., Lyons B., Allison D.E., Kattan M.W., Scher H.I. (2007). Efficacy and safety of single-agent pertuzumab (rhuMAb 2C4), a human epidermal growth factor receptor dimerization inhibitor, in castration-resistant prostate cancer after progression from taxane-based therapy. J Clin Oncol.
15 Albanell J., Montagut C., Jones E.T., Pronk L., Mellado B., Beech J., Gascon P., Zugmaier G., Brewster M., Saunders M.P., Valle J.W. (2008). A phase I study of the safety and pharmacokinetics of the combination of pertuzumab (rhuMab 2C4) and capecitabine in patients with advanced solid tumors. Clin Cancer Res.
16 Friess T., Scheuer W., Hasmann M. (2005). Combination treatment with erlotinib and pertuzumab against human tumor xenografts is superior to monotherapy. Clin Cancer Res.
17 Gordon M.S., Matei D., Aghajanian C., Matulonis U.A., Brewer M., Fleming G.F., Hainsworth J.D., Garcia A.A., Pegram M.D., Schilder R.J., Cohn D.E., Roman L., Derynck M.K., Ng K., Lyons B., Allison D.E., Eberhard D.A., Pham T.Q., Dere R.C., Karlan B.Y. (2006). Clinical activity of pertuzumab (rhuMAb 2C4), a HER dimerization inhibitor, in advanced ovarian cancer: potential predictive relationship with tumor HER2 activation status. J Clin Oncol.
18 Johnson B.E., Janne P.A. (2006). Rationale for a phase II trial of pertuzumab, a HER-2 dimerization inhibitor, in patients with non-small cell lung cancer. Clin Cancer Res.
19 Nahta R., Hung M.C., Esteva F.J. (2004). The HER-2-targeting antibodies trastuzumab and pertuzumab synergistically inhibit the survival of breast cancer cells. Cancer Res.
20 Persson M., Tolmachev V., Andersson K., Gedda L., Sandstrom M., Carlsson J. (2005). [(177)Lu]pertuzumab: experimental studies on targeting of HER-2 positive tumour cells. Eur J Nucl Med Mol Imaging.
21 Persson M., Gedda L., Lundqvist H., Tolmachev V., Nordgren H., Malmstrom P.U., Carlsson J. (2007). [177Lu]pertuzumab: experimental therapy of HER-2-expressing xenografts. Cancer Res.